# ^68^Ga-Labeled alanine derivatives of 1,4,7,10-tetraazacyclododecane-1,7-diacetic acid and 1,4,7,10-tetraazacyclododecane-1,4,7,-triacetic acid

Chemical name: | ^68^Ga-Labeled alanine derivatives of 1,4,7,10-tetraazacyclododecane-1,7-diacetic acid and 1,4,7,10-tetraazacyclododecane-1,4,7,-triacetic acid | [image]
Abbreviated name: | ^68^Ga-21, ^68^Ga-22 | [image]
Synonym: | ^68^Ga-DO2A-alanine, ^68^Ga-DO3A-alanine | [image]
Agent Category: | Others (amino acid) | [image]
Target: | Amino acid transporters | [image]
Target Category: | Transporters | [image]
Method of detection: | Positron emission tomography (PET) | [image]
Source of signal / contrast: | Gallium-68 (^68^Ga) | [image]
Activation: | No | [image]
Studies: | - In vitro; - Rodents | Structures of ^68^Ga-21 and ^68^Ga-22 by Shetty et al. (1).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=amino%20acid%20and%20imaging%20and%20amino%20acid%20transporters)]

The ^68^Ga-labeled alanine derivatives of 1,4,7,10-tetraazacyclododecane-1,7-diacetic acid (DO2A) and 1,4,7,10-tetraazacyclododecane-1,4,7,-triacetic acid (DO3A), abbreviated as ^68^Ga-21 and ^68^Ga-22, respectively, were synthesized by Shetty et al. for positron emission tomography (PET) of cancer cells (1).

Radiolabeled amino acids represent a diverse class of tracers that target the increased amino acid transport in cancer cells (2, 3). To date, >20 distinct amino acid transporters have been identified in mammalian cells, and these transporters differ in terms of substrate specificity, tissue expression patterns, sodium and other ion dependence, pH sensitivity, and transport mechanism (4, 5). Because of increased demand for amino acids in malignant cells, some transporters have been shown to be overexpressed in different types of tumors, and the process of amino acid transport is relatively fast (2, 6, 7). These features make tumor imaging with amino acid tracers possible within 20 min. Indeed, there is growing evidence that radiolabeled amino acids have the potential to overcome some of the limitations of 2-deoxy-2-[^18^F]fluoro-D-glucose ([^18^F]FDG) in tumor imaging, especially in the imaging of primary and recurrent brain tumors, neuroendocrine tumors, and prostate cancers (2, 3, 8). Different studies also showed that radiotracers that target different amino acid transporters exhibit different imaging properties that may provide unique biological information of tumors (1, 2, 7).

The first group of widely investigated amino acids is the analogs of phenylalanine and tyrosine (2, 3). Because of their bulky neutral side chains, these natural amino acids are the substrates of system L transporters and have been proven to be useful for tumor imaging, particularly for brain tumors. The limitation common to most of the natural amino acids is the susceptibility to in vivo metabolism, which decreases tumor specificity and complicates kinetic analysis. Because none of the natural amino acids contain fluorine or iodine, labeling with fluorine-18 or iodine-123 can change the biochemical properties compared to the parent amino acids. These shortcomings associated with natural amino acids can be partially overcome by using non-natural amino acids. Typically, non-natural amino acids are neither metabolized nor readily incorporated into protein in vivo (2, 3, 7). One group of non-natural amino acids is á,á-dialkyl amino acids, which are generated by substituting the á-carbon hydrogen of natural amino acids with a methyl group or other alkyl chains. These amino acids are primarily the substrates of system A transporters. The second group is alicyclic amino acids, which are á,á-dialkyl amino acids with side chains bonded covalently to each other to form a cyclic ring. These amino acids are the substrates of system L transporters. The third group is non-natural proline derivatives, which exhibit different transport selectivity. One challenge in developing amino acid radiotracers is to overcome the low selectivity and the decreased recognition after radiolabeling to specific transporters (1-3). Another challenge is the low uptake of amino acid agents in tumors, which leads to less sensitivity for tumor detection than with [^18^F]FDG (8).

Shetty et al. synthesized a group of ^68^Ga-labeled alanine and lysine derivatives of 1,4,7-triazacyclononane-1,4,7-triacetic acid (NOTA), 1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid (DOTA), DO2A, and DO3A (1, 7). The four bifunctional chelating agents have similar sizes, but they differ in the net charges because of the different numbers of pendent carboxylate arms. The amino acids have been conjugated to one of the carboxylate arms, and the nitrogen atoms in the heterocyclic ring are presumed to coordinate with metals to form chelates. Biodistribution studies and PET imaging indicate the structure–activity relationship of the amino acid derivatives, and the selective uptakes of these compounds by different cancer tissues might provide an insight on the different modes of amino acid uptake by cancer cells (1, 7).

This chapter summarizes the data obtained with ^68^Ga-labeled alanine derivatives: ^68^Ga-21 (^68^Ga-DO2A-alanine) and ^68^Ga-22 (^68^Ga-DO3A-alanine). These alanine derivatives were comparatively analyzed with the corresponding homoalanine derivatives (^68^Ga-23 and ^68^Ga-24, respectively) (1).

### Related Resource Links:

Amino acid transporter-targeted imaging agents in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=amino+acid+transporter+AND+micad%5bbook%5d&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)

Amino acid transporter articles in Online Mendelian Inheritance in Man (OMIM) (http://www.ncbi.nlm.nih.gov/omim/?term=amino+acid+transporter)

Amino acid transporter related clinical trials in ClinicalTrials.gov (http://clinicaltrials.gov/ct2/results?term=amino+acid+transporter)

Amino acid transporter related bioassays in PubChem BioAssay (http://www.ncbi.nlm.nih.gov/pcassay/?term=amino+acid+transporter)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/21055619)]

Shetty et al. synthesized the alanine derivatives, DO2A-alanine (compound 21) and DO3A-alanine (compound 22), by reacting the protected L-serine â-lactone with the compounds 1,4,7,10-tetracyclododecene-1,7-bis(tert-butyl acetate) or 1,4,7,10-tetracyclododecene-1,4,7-tris(tert-butyl acetate), respectively (1).

Radiolabeling of the derivatives with ^68^Ga was carried out at pH 3–4. The labeled reaction mixture was passed through a cartridge to remove the free ^68^Ga^3+^. The labeled agents were analyzed with radiographic thin-layer chromatography. The labeling efficiencies were >97% for both ^68^Ga-21 (^68^Ga-DO2A-alanine) and ^68^Ga-22 (^68^Ga-DO3A-alanine). No free ^68^Ga was found after purification. DOTA without an amino acid residue was labeled with ^68^Ga under the same conditions (^68^Ga-DOTA) and was used as the control for in vitro cell uptake study. The specific activities and stabilities of ^68^Ga-21, ^68^Ga-22, and ^68^Ga-DOTA were not reported (1).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/21055619)]

Cell uptake assays were performed after incubation of Hep3B (human hepatoma) and U87MG (human glioma) cells with 10 ìCi (0.37 MBq) of each agent at 37°C for various times (1). Both ^68^Ga-21 and ^68^Ga-22 exhibited greater uptakes by cells than the control ^68^Ga-DOTA. ^68^Ga-22 showed a higher uptake than ^68^Ga-21 in both cell lines.

Comparative analysis was performed for the cell uptake between alanine and homoalanine derivatives (1). The results showed that all agents (^68^Ga-21 to ^68^Ga-24) exhibited higher uptake than ^68^Ga-DOTA in both cell lines. ^68^Ga-22 had the highest uptake in U87MG cells, whereas ^68^Ga-23 had the highest uptake in Hep3B cells. These results may represent specific uptakes of the amino acid derivatives by cancer cells due to different expressions of various amino acid transporters on cell surfaces. Shetty et al. did not perform blocking experiments, considering that many amino acid derivatives can be transported simultaneously by several different types of transporters and the cell uptake cannot be completely blocked by a single inhibitor (1).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/21055619)]

The biodistribution patterns of ^68^Ga-21 and ^68^Ga-22 were investigated at 10, 30, 60, and 120 min after tail vein injection of each agent (10 ìCi (0.37 MBq)) in mice bearing CT-26 colon cancer xenografts (n = 3–4 mice/time point for each agent) (1). The initial tumor uptakes at 10 min after injection was 2.88% and 3.22% injected dose per gram of tissue (ID/g) for ^68^Ga-21 and ^68^Ga-22, respectively, which then decreased until 60 min (1.05% for ^68^Ga-21 and 2.44% for ^68^Ga-22) and remained almost constant until 120 min after injection (1.08% for ^68^Ga-21 and 2.98% for ^68^Ga-22). The tumor/muscle and tumor/blood ratios peaked at 120 min after injection. The tumor/muscle ratios for ^68^Ga-21 and ^68^Ga-22 were 2.23 and 2.46 at 120 min, respectively. The tumor/blood ratios for ^68^Ga-21 and ^68^Ga-22 were 0.56 and 0.49 at 120 min, respectively.

PET imaging was performed at 30 min after tail vein injection (0.37 MBq (0.01 mCi)) and showed that ^68^Ga-21 had higher tumor uptake and standardized uptake value (SUV) than ^68^Ga-22.

Comparative analysis was also performed for the biodistribution and PET imaging data between alanine and homoalanine derivatives (1). Comparison for the biodistribution showed that all of the alanine and homoalanine derivatives (^68^Ga-21 to ^68^Ga-24) presented high kidney uptake and low liver and intestine uptake, indicating that the major excretion route of these agents is the kidney. The tumor uptake of alanine derivatives (^68^Ga-21 and ^68^Ga-22) was higher than that of homoalanine derivatives (^68^Ga-23 and ^68^Ga-24) at both 30 min and 60 min. However, homoalanine derivatives had higher tumor/nontumor ratios than alanine derivatives at all investigated time points. Similarly, high kidney and bladder activities were observed for all agents in PET imaging. The alanine derivatives showed higher tumor uptakes than the homoalanine derivatives. The SUV for all agents was lower than that of [^18^F]FDG, which might be the result of slow uptake by cancer tissues and rapid excretion through the kidneys. However, tumor/nontumor SUV ratios were high enough to obtain tumor images. ^68^Ga-24 showed the highest tumor/nontumor SUV ratio (3.9 ± 0.3), followed by ^68^Ga-21 (3.1 ± 0.2), ^68^Ga-22 (2.8 ± 0.2), and ^68^Ga-23 (2.3 ± 0.2) at 30 min after injection. No studies of the mechanism were presented.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are currently available.

## References

1 Shetty D., Jeong J.M., Ju C.H., Lee Y.S., Jeong S.Y., Choi J.Y., Yang B.Y., Lee D.S., Chung J.K., Lee M.C. (2010). Synthesis of novel 68Ga-labeled amino acid derivatives for positron emission tomography of cancer cells. Nucl Med Biol.
2 McConathy, J., W. Yu, N. Jarkas, W. Seo, D.M. Schuster, and M.M. Goodman, Radiohalogenated nonnatural amino acids as PET and SPECT tumor imaging agents. Med Res Rev, 2011
3 Laverman P., Boerman O.C., Corstens F.H., Oyen W.J. (2002). Fluorinated amino acids for tumour imaging with positron emission tomography. Eur J Nucl Med Mol Imaging.
4 Ganapathy V., Thangaraju M., Prasad P.D. (2009). Nutrient transporters in cancer: relevance to Warburg hypothesis and beyond. Pharmacol Ther.
5 Goberdhan D.C. (2010). Intracellular amino acid sensing and mTORC1-regulated growth: new ways to block an old target?. Curr Opin Investig Drugs.
6 Fuchs B.C., Bode B.P. (2005). Amino acid transporters ASCT2 and LAT1 in cancer: partners in crime?. Semin Cancer Biol.
7 Shetty D., Jeong J.M., Ju C.H., Kim Y.J., Lee J.Y., Lee Y.S., Lee D.S., Chung J.K., Lee M.C. (2010). Synthesis and evaluation of macrocyclic amino acid derivatives for tumor imaging by gallium-68 positron emission tomography. Bioorg Med Chem.
8 la Fougere C., Suchorska B., Bartenstein P., Kreth F.W., Tonn J.C. (2011). Molecular imaging of gliomas with PET: Opportunities and limitations. Neuro Oncol.